# [O-methyl-^11^C]2-(4-(4-(2-Methoxyphenyl)piperazin-1-yl)butyl)-4-methyl-1,2,4-triazine-3,5(2H,4H)dione

Chemical name: | [O-methyl-^11^C]2-(4-(4-(2-Methoxyphenyl)piperazin-1-yl)butyl)-4-methyl-1,2,4-triazine-3,5(2H,4H)dione
Abbreviated name: | [^11^C]MMP
Synonym: | [^11^C]CUMI-101
Agent category: | Compound
Target: | 5-HT_1A_ serotonin receptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CUMI-101)]

Hydroxytryptamine (5-HT), commonly known as serotonin, has diverse physiological roles as a neurotransmitter in the central nervous system (1). 5-HT is involved in regulation and modulation of sleep, affective and personality behaviors, and pain. It also is a regulator of smooth muscle function and platelet aggregation. The brain cortical 5-HT system has been implicated in several neuropsychiatric disorders, including major depression, anxiety, schizophrenia, and obsessive-compulsive disorder (2, 3). The effects of 5-HT are mediated by as many as seven classes of receptor populations (5-HT_1_ to 5-HT_7_), many of which include several subtypes (4). There are five receptor subtypes within the G-protein–coupled 5-HT_1_ receptor family: 5-HT_1A_, 5-HT_1B_, 5-HT_1D_, 5-HT_1E_, and 5-HT_1F_.

5-HT_1A_ receptors are abundantly present in the hippocampus, entorhinal cortex, frontal cortex, raphe nucleus, and septum; the lowest densities are observed in the basal ganglia, substantia nigra, and cerebellum (5). Some thalamic and hypothalamic nuclei have intermediate densities. 5-HT_1A_ receptors are involved in the mediation of emotion and the function of the hypothalamus. 5-HT_1A_ receptors are implicated in anxiety, depression, hallucinogenic behavior, motion sickness, and eating disorders (6). Thus, there is a need for selective ligands to investigate the pharmacological role of 5-HT_1A_ receptors.

There have been several studies to develop specific 5-HT_1A_ radioligands [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5-HT1a%5BAll%20Fields%5D%20AND%20imaging%5BAll%20Fields%5D)] such as [carbonyl-^11^C]WAY 100635 (http://www.ncbi.nlm.nih.gov/books/NBK23263/), [^18^F]FPWAY (http://www.ncbi.nlm.nih.gov/books/NBK23137/), and [^18^F]MPPF (http://www.ncbi.nlm.nih.gov/books/NBK23391/) for positron emission tomography (PET) imaging. However, none of these antagonists distinguishes between the high- and low-affinity states of the 5-HT_1A_ receptors. The high-affinity state of the receptor is coupled to G-proteins, which mediate the functions of cells by providing intracellular signals. 2-(4-(4-(2-Methoxyphenyl)piperazin-1-yl)butyl)-4-methyl-1,2,4-triazine-3,5(2H,4H)dione (MMP) was reported to be a potent agonist of 5-HT_1A_ receptors (K_i_ = 0.15 nM) (7). This led to the development of [O-methyl-^11^C]2-(4-(4-(2-methoxyphenyl)piperazin-1-yl)butyl)-4-methyl-1,2,4-triazine-3,5(2H,4H)dione ([^11^C]MMP, also known as [^11^C]CUMI-101) as a useful tool for in vivo PET imaging of the 5-HT_1A_ receptor.

### Related Resource Links:

- Chapters in MICAD (5-HT_1A_ (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=5-HT1A+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (5-HT_1A_ (http://www.ncbi.nlm.nih.gov/gene/3350))
- Articles in Online Mendelian Inheritance in Man (OMIM) (5-HT_1A_ (http://www.ncbi.nlm.nih.gov/omim/109760))
- Clinical trials (5-HT_1A_ (http://www.clinicaltrials.gov/ct2/results?term=5-HT1A))
- Drug information in Food and Drug Administration (5-HT_1A_ (http://google2.fda.gov/search?q=5-HT1a&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=8&y=1))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CUMI-101%20and%20synthesis)]

The radiosynthesis of [^11^C]MMP, reported by Kumar et al. (7), involved standard ^11^C-methylation of the corresponding desmethyl precursor 2-(4-(4-(2-hydroxyphenyl)piperazin-1-yl)butyl)-4-methyl-1,2,4-triazine-3,5-(2H,4H)-dione with [^11^C]CH_3_OTf in acetone in the presence of NaOH. The reported overall radiochemical yield of the radiosynthesis was 30 ± 5% at the end of synthesis (EOS), the specific radioactivity was 96 ± 19 TBq/mmol (2,600 ± 500 Ci/mmol), and the radiochemical purity was >98%. The total synthesis time was 30 min at EOS.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CUMI-101%20and%20in%20vitro)]

Kumar et al. (7) performed in vitro competition binding studies with [^3^H]8-OH-DPAT in bovine hippocampus membranes. MMP had a K_i_ of 0.15 ± 0.05 nM. The affinity of MMP for various biogenic amines, brain receptors, and transporters was determined to be >45 times lower than that of MMP. Agonist properties of MMP on 5-HT_1A_ receptors were evaluated using [^35^S]-labeled guanosine gamma thio-phosphate ([^35^S]GTPγS) binding in membranes of Chinese hamster ovary (CHO) cells stably expressing the human 5-HT_1A_ receptors. MMP produced a dose-dependent increase in [^35^S]GTPγS binding. Maximal MMP-stimulated [^35^S]GTPγS binding was 80% of that seen with 5-HT. The maximum binding fraction for MMP (0.10 nM) was comparable to that for 5-HT (0.56 nM). There was a measurable free fraction of [^11^C]MMP in baboon (59%) and human (37%) plasma.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CUMI-101%20and%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CUMI-101%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CUMI-101%20and%20nonhuman%20primate)]

PET imaging was used to study radioactivity accumulation in baboon brains after intravenous injection of 185 MBq (5 mCi) of [^11^C]MMP (7). Various brain regions exhibited rapid accumulation in 3–13 min with gradual decreases thereafter. [^11^C]MMP PET images (up to 120 min after injection) displayed radioactivity concentrations (tissue/cerebellum ratio) that followed a rank order: the hippocampus (6.25), insular cortex (5.25) cingulate gyrus (4.75), prefrontal cortex (4.0), amygdala (3.75), raphe nucleus (3.0), thalamus (2.0), and cerebellum (1.0) at 105 min. Pretreatment with the antagonist WAY 100635 (0.25 mg/kg) or the agonist 8-OH-DPAT (2 mg/kg) 30 min prior to the injection of [^11^C]MMP markedly reduced the radioactivity by ~70% in the hippocampus, cingulate gyrus and prefrontal cortex. There was a minor blockade effect in the cerebellum. After injection of [^11^C]MMP, 84%, 43%, 32%, and 24% of the total plasma radioactivity was intact at 4, 30, 60, and 90 min, respectively. Only hydrophilic metabolites were detected.

Milak et al. (8) performed [^11^C]CUMI-101PET scans in the brain of two male baboons. Scanning time of 100 min was adequate and that for the region-of-interest analysis, the likelihood estimation in graphical analysis (LEGA) model provided the best results. The median test–retest percentage difference for binding potential (BP_F_) was 11.15% ± 4.82% across all regions. Pre-administration of WAY100635 and 8-OH-DPAT resulted in 87% and 76% average reductions in BP_F_ values across all regions of interests, respectively. All metabolites were more polar than ^11^C-CUMI-101, and no significant change in metabolites was observed in the blocking studies. The free fraction in the plasma was 59% ± 3%.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CUMI-101%20and%20human)]

Milak et al. (9) performed [^11^C]CUMI-101 PET brain scans of seven human volunteers. Scanning time of 120 min was found to be adequate for the region-of-interest analysis. The LEGA model provided the best results with the median test–retest percentage difference for BP_F_ values was 9.9% ± 5.6% across all regions. The free fraction in the plasma was 30% ± 3%. The BP_F_ values for entorhinal cortex, hippocampus, temporal lobe, amygdala, insular cortex, cingulate, prefrontal cortex, raphe, and occipital lobe were 32.62, 31.66, 28.61, 25.50, 21.20, 18.48, 13.69, 12.42, and 9.70 mL/cm^3^, respectively.

Hines et al. (10) performed PET imaging studies to determine biodistribution and dosimetry of 428 ± 84 MBq (11.56 ± 2.27 mCi, 5.0 ± 1.0 nmol) [^11^C]CUMI-101 in nine healthy volunteers. The brain had high accumulation (~11% of injected dose (ID)) at 10 min. Although liver had the highest uptake (~35% ID at 120 min), excretion of radioactivity was not visible in gall bladder or intestine during the scanning session. Organs with the highest radiation doses were the pancreas (32.0 µSv/MBq, 118.4 mrem/mCi), liver (18.4 µSv/MBq, 68.1 mrem/mCi), and spleen (14.5 µSv/MBq, 53.7 mrem/mCi). The effective dose for ^11^C-CUMI-101 was 5.3 ± 0.5 µSv/MBq (19.5 ± 2.2 mrem/mCi).

## NIH Support

P50 MH62185, R21 MH077161, K08 MH76258, MH62185,

## References

1 Lucki I. (1998). The spectrum of behaviors influenced by serotonin. Biol Psychiatry.
2 Fletcher A., Cliffe I.A., Dourish C.T. (1993). Silent 5-HT1A receptor antagonists: utility as research tools and therapeutic agents. Trends Pharmacol Sci.
3 Hoyer D., Clarke D.E., Fozard J.R., Hartig P.R., Martin G.R., Mylecharane E.J., Saxena P.R., Humphrey P.P. (1994). International Union of Pharmacology classification of receptors for 5-hydroxytryptamine (Serotonin). Pharmacol Rev.
4 Lanfumey L., Hamon M. (2004). 5-HT1 receptors. Curr Drug Targets CNS Neurol Disord.
5 Pazos A., Probst A., Palacios J.M. (1987). Serotonin receptors in the human brain--III. Autoradiographic mapping of serotonin-1 receptors. Neuroscience.
6 Cowen P.J. (2000). Psychopharmacology of 5-HT(1A) receptors. Nucl Med Biol.
7 Kumar J.S., Prabhakaran J., Majo V.J., Milak M.S., Hsiung S.C., Tamir H., Simpson N.R., Van Heertum R.L., Mann J.J., Parsey R.V. (2007). Synthesis and in vivo evaluation of a novel 5-HT(1A) receptor agonist radioligand [O-methyl- (11)C]2-(4-(4-(2-methoxyphenyl)piperazin-1-yl)butyl)-4-methyl-1,2,4-triazi ne-3,5(2H,4H)dione in nonhuman primates. Eur J Nucl Med Mol Imaging.
8 Milak M.S., Severance A.J., Ogden R.T., Prabhakaran J., Kumar J.S., Majo V.J., Mann J.J., Parsey R.V. (2008). Modeling considerations for 11C-CUMI-101, an agonist radiotracer for imaging serotonin 1A receptor in vivo with PET. J Nucl Med.
9 Milak M.S., DeLorenzo C., Zanderigo F., Prabhakaran J., Kumar J.S., Majo V.J., Mann J.J., Parsey R.V. (2010). In vivo quantification of human serotonin 1A receptor using 11C-CUMI-101, an agonist PET radiotracer. J Nucl Med.
10 Hines C.S., Liow J.S., Zanotti-Fregonara P., Hirvonen J., Morse C., Pike V.W., Innis R.B. (2011). Human biodistribution and dosimetry of (1)(1)C-CUMI-101, an agonist radioligand for serotonin-1a receptors in brain. PLoS One.